# ^99m^Tc-Methyl diphosphonate

Chemical name: | ^99m^Tc-Methyl diphosphonate
Abbreviated name: | ^99m^Tc -MDP
Synonym: | ^99m^Tc -Methylene diphosphonate, Technetium 99mTc Medronate
Agent Category: | Compound
Target: | Type 2 class of aminoacyl-tRNA synthetases
Target Category: | Enzymes
Method of detection: | Single photon emission computed tomography (SPECT); planar gamma imaging
Source of signal / contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Non-human primates; - Humans | Structure of ^99m^Tc-MDP. Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc-MDP)]

Invasive procedures are often necessary to treat internal bone injuries or disorders. Therefore it is important for individuals providing treatment to accurately diagnose the disorder to provide the most suitable therapy before subjecting the patient to any invasive procedures. Bone injuries are often investigated either by magnetic resonance imaging (MRI) or single-photon emission computed tomography (SPECT) scans using radionuclides (1). The SPECT technique is based on imaging of radionuclides and the fact that certain elements or compounds concentrate selectively in specific tissue. Compared to other imaging techniques, e.g., planar scintigraphy, SPECT provides detailed information about the anatomy and physiological state of the bone (1, 2). Bone SPECT has been used to detect early osteonecrosis of the femoral head in renal transplant patients (3), to investigate internal derangement and stress fractures of the knee (4, 5) and also to monitor bone metastasis in breast (6), gastric (7), and prostate (8) cancers. Imaging with ^99m^Tc-methylene diphosphonate (^99m^Tc-MDP) is the initial method of choice to detect skeletal metastases in cancer patients (9).

For SPECT of the bone, metastable technetium (^99m^Tc) is tagged onto a phosphonate compound such as MDP to generate ^99m^Tc-MDP, which selectively concentrates in the bone. Although accumulation of ^99m^Tc-MDP in the bone is caused by its chemical adsorption onto, and into, the crystalline structure of hydroxyapatite (10), but the enzyme aminoacyl-tRNA synthetase is believed to convert it into ATP analogues that inhibit any ATP-dependent enzymes and result in cellular apoptosis (11). For scintigraphy the labeled compound is administered intravenously to the patient and SPECT is subsequently performed after suitable time periods.

^99m^Tc-MDP has been approved by the US Food and Drug Administration as an imaging agent to investigate osteogenesis and is commercially available in kit form (12).Results obtained with any new radiolabeled compound being evaluated for bone imaging in clinical trials (http://clinicaltrials.gov/ct2/results?term=99mTc-MDP) are compared to those obtained with ^99m^Tc-MDP.

### Other sources of information:

Protein (http://www.ncbi.nlm.nih.gov/protein/NP_446209.1) and mRNA (http://www.ncbi.nlm.nih.gov/nuccore/NM_053757.1) sequence of rat aminoacyl-tRNA synthetase

Gene information (http://www.ncbi.nlm.nih.gov/sites/nuccore?Db=gene&DbFrom=nuccore&Cmd=Link&LinkName=nuccore_gene&IdsFromResult=75832034) regarding rat aminoacyl-tRNA synthetase (GeneID: 114632) (Source: Entrez Gene)

Aminoacyl tRNA synthetase in Online Mendelian Inheritance in Man (OMIM) (http://www.ncbi.nlm.nih.gov/omim?term=aminoacyl%20tRNA%20synthetase)

Structure (http://www.ncbi.nlm.nih.gov/Structure/mmdb/mmdbsrv.cgi?uid=80673) of human cytosolic phenylalanyl-tRNA synthase (Source: NCBI)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-MDP%20synthesis)]

Because synthesis of ^99m^Tc-MDP can be performed at room temperature, a kit for its preparation immediately before use is commercially available (12). The kit includes a vial containing a lyophilized, sterile, nonpyrogenic, and nonradioactive mixture of medronic acid, stannous chloride dehydrate, and p-aminobenzoic acid that is packed under nitrogen. Prior to lyophilization, pH of the mixture is adjusted to between 6.5 and 7.5 with hydrochloric acid or sodium hydroxide. To prepare ^99m^Tc-MDP, sodium pertechnetate (^99m^Tc), available as a sterile nonpyrogenic preparation from commercial sources, is injected into the vial containing the lyophilized mixture. To mix the solution, the vial is swirled gently until the contents are completely dissolved. According to the manufacturer, the labeling is rapid and quantitative. The maximum recommended amount of ^99m^Tc to add to the vial is 500 mCi (18.5 GBq). The product information and insert can be viewed at the manufacturers website (http://usa.braccoimaging.com/images/stories/pdf/nuclear/mdp-bracco/MDP-Bracco8.5x11.pdf).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-MDP%20in%20vitro)]

The mechanism of ^99m^Tc-MDP accumulation in bone was investigated in mice calvaria, osteoblast-like cells, collagen sponges, and hydroxyapatite powder (10). Uptake of the label was observed only in cells growing out from the calvaria fragments and in calvaria fragments fixed with ethanol. Pyrophosphate and EDTA reduced the accumulation of ^99m^Tc-MDP on the calvaria fragments. No correlation was observed between the number of osteoblast-like cells and the accumulation of ^99m^Tc-MDP. No accumulation of ^99m^Tc-MDP was seen in the collagen sponges. These observations suggest that ^99m^Tc-MDP accumulates on the bone by chemical adsorption and incorporation into the hydroxyapatite structure.

The uptake of ^99m^Tc-MDP was investigated in two rat tibial bone models (13). In one model, the bone had a specific injury, and in the other there was osteomyelitis. Both models were evaluated by scintigraphy and ^31^P magnetic resonance spectroscopy for pH, mineral phosphate/creatinine phosphate ratio (Pi/PCr), and ATP/PCr ratio over a three-week period. In both models the ^99m^Tc-MDP uptake peaked at ~one week and gradually decreased thereafter. With the scintigram the injured bone demonstrated distinct uptake, but there was a diffused uptake in the osteomyelitis model. Only the osteomyelitis model showed a significant change in pH and ATP/PCr, but not Pi/Cr. This indicated that the accumulation of ^99m^Tc-MDP in the bone was affected by the disease type and environmental factors such as pH and phosphate concentration.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc-MDP+rodentia)]

The uptake of ^99m^Tc-MDP and ^32^P incorporation was used as a measure of bone healing during endosteal healing with titanium, hydroxyapatite (these are considered bone-bonding materials), or stainless steel (does not bind to bone) implants in rat tibial bone after bone marrow ablation (14). The distribution of ^99m^Tc-MDP and ^32^P was observed to vary according to the implant, which indicated that the implants influenced bone healing. The investigators suggest that the distribution and uptake of the two labels may be useful parameters to study bone bonding.

The effect of mitomycin-C, a drug used to treat cancer, on the biodistribution of ^99m^Tc-MDP in mice was investigated (15). Although the drug affected radioactivity uptake in the stomach, ovary, pancreas, uterus, kidneys, spleen, thymus, heart, liver, and lungs, no significant change was observed in thyroid, brain, or bones of the animals. The investigators concluded that mitomycin-C did not interfere with ^99m^Tc-MDP bone SPECT; however, because it changed the uptake in some organs, any hot spots should be examined carefully for diagnosis.

The whole-body (WB) retention of ^47^CaCl and ^99m^Tc-MDP was investigated in three bone disease models (osteomalacic, steroid-induced osteoporosis, and osteoporosis) in rats (16). The three disease models showed marked differences in WB retention of the two radiopharmaceuticals after 24 h of administration. On the basis of these observations, the investigators suggest that these radiopharmaceuticals can be used to differentiate the various bone diseases prior to detection of radiological changes in the animal models.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-MDP%20non-primate%20mammals)]

Drost et al. (17) investigated the use of ^99m^Tc-MDP scintigraphy to determine the onset time frame, distribution, and appearance of bone lesions in dogs infected with Hepatozoon americanum oocytes. These protozoans proliferate on the long bones, pelvis, vertebrae, and skull of the animals. The investigators described the appearance of the lesions and concluded that scintigraphy can be used to evaluate the H. americanum lesions in the animals.

Scintigraphy using ^99m^Tc-MDP was performed on lame dogs after clinical examination; radiography and synovial fluid analysis could not localize the cause of lameness to a specific area of pain (18). After bone scintigraphy, the investigators concluded that the highly sensitive and relatively specific uptake of the label could be used to localize and characterize, or exclude, the skeletal lesions that caused lameness in most dogs examined in this study.

The effect of ^99m^Tc-MDP and ^99m^Tc-dicarboxypropane diphosphonate (^99m^Tc-DPD) on bone scan image quality and time in dogs with osteoarthritis was evaluated (19). The investigators observed that both labels yielded similar results for radioactivity uptake and image quality; however, ^99m^Tc-DPD was more efficient than ^99m^Tc-MDP in reducing the overall time of scintigraphy.

Some SPECT work has also been done to diagnose tooth infections (20) and paranasal disorders (21) in horses.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-MDP%20non-human%20primates)]

Scintigraphy with ^99m^Tc-MDP was used to evaluate the healing of long bone fractures in baboons (22). The investigators concluded that ^99m^Tc-MDP scintigraphy was an accurate technique to investigate the physiological activity of bones. The same investigators also concluded that this technique was a valuable diagnostic tool in traumatic orthopedic surgery for the quantitative and qualitative evaluation of long bone healing in these animals (23).

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

Several investigators have shown that ^99m^Tc-MDP scans (WB bone or specific body parts) can be used to monitor, diagnose, and detect a variety of human diseases (24-27).

A retrospective study assessed the use of WB bone scintigraphy (WB BSc) with ^99m^Tc-MDP to monitor the effect of biphosphonate treatment in patients with breast cancer and bone metastasis (6). After compiling the results the investigators concluded that WB BSc with ^99m^Tc-MDP was a reliable method to assess this therapy in the treatment planning of breast cancer patients. Binnie et al. have suggested the use of pre-therapeutic ^99m^Tc-MDP bone scans to plan targeted radionulide therapy for bone metastases caused by prostate cancer (28). On the other hand, it has been suggested that ^18^F-fluoride positron emission tomography/computed tomography is a more sensitive and specific method than ^99m^Tc-MDP planar scintigraphy to detect bone metastases in prostate cancer patients (8). The use of bone scintigraphy in common osteolytic tumors has been discussed and illustrated by Wang et al. (29).

A WB BSc with ^99m^Tc-MDP of a man with medullary carcinoma of the thyroid revealed hepatic metastases that were later confirmed with a computed tomography scan (24), which indicated that WB BSc with ^99m^Tc-MDP can be used to detect hepatic metastasis. In another study, WB BSc with ^99m^Tc-MDP revealed an unusually extensive metastatic disease in the abdominal region, without lung involvement, in a patient who underwent intensive chemotherapy (25). The investigators recommend that patients with osteosarcoma who have signs of intestinal or abdominal obstruction should be subject to bone scintigraphy to reveal any unexpected metastatic foci.

^99m^Tc-MDP scintigraphy has also been used to detect femoral head avascular osteonecrosis (26) and the characteristic lesions of Erdheim-Chester disease (27).

## Supplemental Information

[Disclaimer]

No information is currently available.

## References

1 Prasad V.R. (2006). Derangement of knee: role of radionuclide imaging in the diagnosis. Imaging Decisions MRI.
2 Kajan Z.D., Motevasseli S., Nasab N.K., Ghanepour H., Abbaspur F. (2006). Assessment of growth activity in the mandibular condyles by single-photon emission computed tomography (SPECT). Aust Orthod J.
3 Ryu J.S., Kim J.S., Moon D.H., Kim S.M., Shin M.J., Chang J.S., Park S.K., Han D.J., Lee H.K. (2002). Bone SPECT is more sensitive than MRI in the detection of early osteonecrosis of the femoral head after renal transplantation. J Nucl Med.
4 So Y., Chung J.K., Seong S.C., Sohn Y.J., Kang H.S., Lee D.S., Lee M.C. (2000). Usefulness of 99Tcm-MDP knee SPET for pre-arthroscopic evaluation of patients with internal derangements of the knee. Nucl Med Commun.
5 Yildirim M., Gursoy R., Varoglu E., Oztasyonar Y., Cogalgil S. (2004). 99mTc-MDP bone SPECT in evaluation of the knee in asymptomatic soccer players. Br J Sports Med.
6 Chavdarova L., Piperkova E., Tsonevska A., Timcheva K., Dimitrova M. (2006). Bone scintigraphy in the monitoring of treatment effect of bisphosphonates in bone metastatic breast cancer. J Buon.
7 Choi C.W., Lee D.S., Chung J.K., Lee M.C., Kim N.K., Choi K.W., Koh C.S. (1995). Evaluation of bone metastases by Tc-99m MDP imaging in patients with stomach cancer. Clin Nucl Med.
8 Even-Sapir E., Metser U., Mishani E., Lievshitz G., Lerman H., Leibovitch I. (2006). The detection of bone metastases in patients with high-risk prostate cancer: 99mTc-MDP Planar bone scintigraphy, single- and multi-field-of-view SPECT, 18F-fluoride PET, and 18F-fluoride PET/CT. J Nucl Med.
9 Uematsu T., Yuen S., Yukisawa S., Aramaki T., Morimoto N., Endo M., Furukawa H., Uchida Y., Watanabe J. (2005). Comparison of FDG PET and SPECT for detection of bone metastases in breast cancer. AJR Am J Roentgenol.
10 Kanishi D. (1993). 99mTc-MDP accumulation mechanisms in bone. Oral Surg Oral Med Oral Pathol.
11 Roelofs A.J., Thompson K., Gordon S., Rogers M.J. (2006). Molecular mechanisms of action of bisphosphonates: current status. Clin Cancer Res.
12 . Bracco, Kit for the preparation of technetium Tc 99m Medronate. 2006, Bracco Diagnostics Inc.: Princeton, NJ 08543.
13 Okamoto Y.M. (1997). Mechanism of accumulation of 99mTc-MDP to bone: correlation of in vivo data with in vitro data. Radiat Med.
14 Sela J., Shani J., Kohavi D., Soskolne W.A., Itzhak K., Boyan B.D., Schwartz Z. (1995). Uptake and biodistribution of 99mtechnetium methylene-[32P] diphosphonate during endosteal healing around titanium, stainless steel and hydroxyapatite implants in rat tibial bone. Biomaterials.
15 Gomes M.L., de Souza Braga A.C., de Mattos D.M., de Souza Freitas R., Boasquevisque E.M., Bernardo-Filho M. (1998). The effect of mitomycin-C on the biodistribution of 99Tcm-MDP in Balb/c mice. Nucl Med Commun.
16 Seto H., Ihara F., Futatsuya R., Kamei T., Kakishita M., Noda M. (1993). Simultaneous measurements of twenty-four-hour whole-body retention of 47Ca-chloride and 99mTc-MDP: early differentiation of metabolic bone diseases in rat models. Nucl Med Biol.
17 Drost W.T., Cummings C.A., Mathew J.S., Panciera R.J., Ko J.C. (2003). Determination of time of onset and location of early skeletal lesions in young dogs experimentally infected with Hepatozoon americanum using bone scintigraphy. Vet Radiol Ultrasound.
18 Schwarz T., Johnson V.S., Voute L., Sullivan M. (2004). Bone scintigraphy in the investigation of occult lameness in the dog. J Small Anim Pract.
19 Lee J.Y., Lee W.G., Kim J.H., Kang S.S., Bae C.S., Koong S.S., Choi S.H. (2005). Comparison of the effect of 99mTc-DPD and 99mTc-MDP on experimentally-induced osteoarthritis in the stifle joint of the dog. In Vivo.
20 Weller R., Livesey L., Maierl J., Nuss K., Bowen I.M., Cauvin E.R., Weaver M., Schumacher J., May S.A. (2001). Comparison of radiography and scintigraphy in the diagnosis of dental disorders in the horse. Equine Vet J.
21 Barakzai S., Tremaine H., Dixon P. (2006). Use of scintigraphy for diagnosis of equine paranasal sinus disorders. Vet Surg.
22 Dormehl I.C., Mennen U., Goosen D.J. (1982). A technique to evaluate bone healing in non-human primates using sequential 99mTc-methylene diphosphonate scintigraphy. Nuklearmedizin.
23 Mennen U., Dormehl I.C., Goosen D.J. (1985). Evaluation of the healing process of bone fractures in the non-human primate using sequential 99mTc-methylene diphosphonate scintigraphy. S Afr J Surg.
24 Ali I., Johns W., Gupta S.M. (2006). Visualization of hepatic metastases of medullary thyroid carcinoma on Tc-99m MDP bone scintigraphy. Clin Nucl Med.
25 Karacalioglu O., Ilgan S., Kuzhan O., Emer O., Ozguven M. (2006). Disseminated metastatic disease of osteosarcoma of the femur in the abdomen: unusual metastatic pattern on Tc-99m MDP bone scan. Ann Nucl Med.
26 Lee E.J., Lee K.H., Huh W.S., Yoon J.K., Chung H.W., Choi J.Y., Choe Y.S., Choi Y., Oh H.Y., Kim B.T. (2006). Incidence and radio-uptake patterns of femoral head avascular osteonecrosis at 1 year after renal transplantation: a prospective study with planar bone scintigraphy. Nucl Med Commun.
27 Namwongprom S., Nunez R., Kim E.E., Macapinlac H.A. (2007). Tc-99m MDP bone scintigraphy and positron emission tomography/computed tomography (PET/CT) imaging in Erdheim-Chester disease. Clin Nucl Med.
28 Binnie D., Divoli A., McCready V.R., Dearnaley D., Flux G. (2005). The potential use of 99mTc-MDP bone scans to plan high-activity 186Re-HEDP targeted therapy of bony metastases from prostate cancer. Cancer Biother Radiopharm.
29 Wang K., Allen L., Fung E., Chan C.C., Chan J.C., Griffith J.F. (2005). Bone scintigraphy in common tumors with osteolytic components. Clin Nucl Med.